# ^99m^Tc-Diethylenetriamine pentaacetic acid–lactosyl human serum albumin

Chemical name: | ^99m^Tc-Diethylenetriamine pentaacetic acid–lactosyl human serum albumin
Abbreviated name: | ^99m^Tc-LACTAL
Synonym:
Agent Category: | Proteins
Target: | Asialoglycoprotein receptors (ASGP-Rs)
Target Category: | Receptors
Method of detection: | Planar gamma imaging; single-photon emission computed tomography (SPECT)
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=liver+function+and+asialoglycoprotein+receptors+and+imaging)]

The ^99m^Tc-diethylenetriamine pentaacetic acid (DTPA)–lactosyl human serum albumin (HSA), abbreviated as ^99m^Tc-LACTAL, is a radiolabeled lactosylated ligand developed by Chaumet-Riffaud et al. for noninvasive assessment of liver function by targeting asialoglycoprotein receptors (ASGP-Rs) on the surface of hepatocytes (1).

Precise assessment of liver functional reserve has long been a critical issue in the diagnosis and treatment of liver diseases (2, 3). Various biochemical tests and imaging studies, such as laboratory tests, clearance and tolerance tests, functional imaging, and volumetric tests, have been designed to assess liver function (2, 4). Because of the complexity of liver function, there is no single method that is capable of assessing the overall liver function. Recently, an imaging technique involving ASGP-Rs and radiolabeled galactosylated ligands has been intensively investigated and shows great promise. ASGP-Rs are localized on the surface of hepatocytes and play a major role in the hepatic clearance of serum ASGPs with a galactosyl moiety. After binding with ASGP-Rs, ASGPs are endocytosed, degraded in the lysosomes, and excreted into the bile. In the settings of various liver diseases, both the number of ASGP-Rs and their function are significantly reduced (1-3). The blood clearance and binding with ASGP-Rs for a galactosylated ligand are thus considered to directly reflect the numbers of both functional ASGP-Rs and hepatocytes and can be used as indicators of liver functional reserve. In the literature, several galactosylated ligands have been reported, including Cy5.5-DTPA-galactosyl-dextran, ^99m^Tc-galactosyl-neoglycoalbumin (^99m^Tc-NGA), ^99m^Tc-DTPA-galactosyl-HSA (^99m^Tc-GSA (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=GSATc99m)), ^99m^Tc-galactosyl-methylated chitosan (^99m^Tc-GMC (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=GMC-99mTc)), ^99m^Tc-HYNIC-galactosyl-chitosan (^99m^Tc-HGC (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=HGC-HYNIC99mTc)), ^99m^Tc-DTPA-superparamagnetic iron oxide-lactobionic acid nanoparticles (^99m^Tc-DTPA-SPION-LBA (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=LBA-SPION-99mTc)), and ^18^F-neoglycoalbumin ([^18^F]FNGA (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=NGA18F)) (5-11). Of them, ^99m^Tc-GSA has been approved for clinical use in Japan. Imaging with ASGP-R–targeted ligands has provided a more precise assessment of the liver functional reserve than other measurements (e.g., biochemical tests, indocyanine green retention, and the Child-Pugh scoring system) (12). However, the synthetic procedures of these ligands, as noted by Chaumet-Riffaud et al., have a number of limitations: long reaction times, reduction of structural disulfide bonds, alterations of the net charge of the protein, or reactions involving toxic reagents such as sodium cyanoborohydride for reductive amination (1). Chaumet-Riffaud et al. developed an alternative process to prepare ^99m^Tc-LACTAL with maleimido-derivatized reagents. Preclinical studies validated the use of ^99m^Tc-LACTAL as a radiopharmaceutical agent for liver function imaging (1).

### Related Resource Links:

- Nucleotide (http://www.ncbi.nlm.nih.gov/nucleotide/?term=asialoglycoprotein+receptors) and protein (http://www.ncbi.nlm.nih.gov/protein/?term=asialoglycoprotein+receptors) information of asialoglycoprotein receptors
- Articles on asialoglycoprotein receptors in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=asialoglycoprotein+receptors)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20201600)]

Chaumet-Riffaud et al. described the synthesis of ^99m^Tc-LACTAL in detail (1). The process included maleimidopropyl-lactose (yield = 60%) and maleimidopropyl-DTPA (yield = 51%) synthesis, HSA modification, and ^99m^Tc chelating. Preparation of the LACTAL was finished in a quick single-step reaction involving maleimido-derivatized reagents (for 1 h at room temperature). The lactose and DTPA derivatives were introduced on the ε-amino groups of the HSA lysines. The amount of DTPA was 5 ± 1 DTPA/HSA (mol/mol), and the lactose concentration was 30 ± 3 lactose/HSA (mol/mol). The estimated mass of LACTAL was 93 kDa, which corresponded to 29 lactose units and 5 DTPA units.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20201600)]

Chaumet-Riffaud et al. checked the stability of the LACTAL solution after storage for 1 year at 4ºC and for 32 months at the lyophilized status (1). There were no differences from freshly prepared material, no aggregates were observed, and the imaging properties were identical. The ^99m^Tc-LACTAL solution was stable at room temperature for 20 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20201600)]

Chaumet-Riffaud et al. performed imaging studies in male Wistar rats (n = 9) with ^99m^Tc-LACTAL and a small-animal dedicated gamma camera (1). ^99m^Tc-LACTAL was injected intravenously through the penis vein. After injection, ^99m^Tc-LACTAL distributed rapidly to the highly vascularized organs. An early and predominantly hepatic uptake was observed, with a plateau that was reached within 2–6 min and continued for at least 20 min. After 30 min, the liver uptake began to decrease, and ^99m^Tc-LACTAL was excreted largely from the bile ducts.

Chaumet-Riffaud et al. also performed biodistribution studies in male mice with ^99m^Tc-LACTAL and a gamma scintillation counter (1). The ^99m^Tc-LACTAL was injected via the tail vein. Mice were then euthanized (n = 3 mice at 10, 30, and 90 min, respectively) and organs were collected. Non-lactosylated ^99m^Tc-HSA was used as a control. The biodistribution data were consistent with the imaging results in rats. The liver uptake was very early and intense with 51.3 ± 4.27, 36.7 ± 6.68, and 24.3 ± 3.19% injected dose per gram (ID/g) at 10, 30, and 90 min, respectively. The activity in other organs (spleen, heart, lungs, and kidneys) was much lower, suggesting the specificity of ^99m^Tc-LACTAL for hepatic ASGP-Rs. Blood levels were also very low (after 10 min), indicating rapid plasma clearance. The radioactivity values in blood were 1.98 ± 0.60, 0.59 ± 0.24, and 0.82 ± 0.03% ID/g at 10, 30, and 90 min, respectively. The hepatic uptake for the control non-lactosylated ^99m^Tc-HSA (5.10 ± 1.55% ID/g at 1 h after injection) was much lower than the blood activity (35.3 ± 4.04% ID/g at 1 h after injection), suggesting that this tracer remained mainly in the intravascular compartment.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Chaumet-Riffaud P., Martinez-Duncker I., Marty A.L., Richard C., Prigent A., Moati F., Sarda-Mantel L., Scherman D., Bessodes M., Mignet N. (2010). Synthesis and application of lactosylated, 99mTc chelating albumin for measurement of liver function. Bioconjug Chem.
2 Schneider P.D. (2004). Preoperative assessment of liver function. Surg Clin North Am.
3 Hoefs J.C., Chen P.T., Lizotte P. (2006). Noninvasive evaluation of liver disease severity. Clin Liver Dis.
4 de Graaf W., Bennink R.J., Vetelainen R., van Gulik T.M. (2010). Nuclear imaging techniques for the assessment of hepatic function in liver surgery and transplantation. J Nucl Med.
5 Huang G., Diakur J., Xu Z., Wiebe L.I. (2008). Asialoglycoprotein receptor-targeted superparamagnetic iron oxide nanoparticles. Int J Pharm.
6 Jeong J.M., Hong M.K., Kim Y.J., Lee J., Kang J.H., Lee D.S., Chung J.K., Lee M.C. (2004). Development of 99mTc-neomannosyl human serum albumin (99mTc-MSA) as a novel receptor binding agent for sentinel lymph node imaging. Nucl Med Commun.
7 Kim E.M., Jeong H.J., Kim S.L., Sohn M.H., Nah J.W., Bom H.S., Park I.K., Cho C.S. (2006). Asialoglycoprotein-receptor-targeted hepatocyte imaging using 99mTc galactosylated chitosan. Nucl Med Biol.
8 Sugahara K., Togashi H., Takahashi K., Onodera Y., Sanjo M., Misawa K., Suzuki A., Adachi T., Ito J., Okumoto K., Hattori E., Takeda T., Watanabe H., Saito K., Saito T., Sugai Y., Kawata S. (2003). Separate analysis of asialoglycoprotein receptors in the right and left hepatic lobes using Tc-GSA SPECT. Hepatology.
9 Yang W., Mou T., Peng C., Wu Z., Zhang X., Li F., Ma Y. (2009). Fluorine-18 labeled galactosyl-neoglycoalbumin for imaging the hepatic asialoglycoprotein receptor. Bioorg Med Chem.
10 Yang W., Mou T., Zhang X., Wang X. (2010). Synthesis and biological evaluation of (99m)Tc-DMP-NGA as a novel hepatic asialoglycoprotein receptor imaging agent. Appl Radiat Isot.
11 Vera D.R., Hall D.J., Hoh C.K., Gallant P., McIntosh L.M., Mattrey R.F. (2005). Cy5.5-DTPA-galactosyl-dextran: a fluorescent probe for in vivo measurement of receptor biochemistry. Nucl Med Biol.
12 Kokudo N., Vera D.R., Makuuchi M. (2003). Clinical application of TcGSA. Nucl Med Biol.